# ^99m^Tc-Gly-Gly-Cys-(Arg)_3_-bombesin(2-14)-NH_2_

Chemical name: | ^99m^Tc-Gly-Gly-Cys-(Arg)_3_-bombesin(2-14)-NH_2_ | [image]
Abbreviated name: | ^99m^Tc-BN-A | [image]
Synonym: | | [image]
Agent Category: | Peptides | [image]
Target: | Gastrin-releasing peptide receptors (GRPR) | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of ^99m^Tc-BN-A and ^99m^Tc-BN-O (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=bombesin%5bTitle%5d%20AND%20imaging%5bTitle%5d%20AND%20gastrin-releasing%5bTitle%5d%20AND%20peptide%5bTitle%5d%20AND%20receptor%5bTitle%5d)]

^99m^Tc-Gly-Gly-Cys-(Arg)_3_-bombesin(2-14)-NH_2_, abbreviated as ^99m^Tc-BN-A, is an analog of the bombesin (BN) peptide, which was synthesized by Liolios et al. for imaging of tumors that express gastrin-releasing peptide receptors (GRPR) (1).

BN is an amphibian neuropeptide consisting of 14 amino acids (pGlu-Gln-Arg-Leu-Gly-Asn-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_) (2, 3). It shares an identical C-terminal region (-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_) with gastrin-releasing peptide (GRP), which is responsible for receptor binding and signal transduction (4, 5). There are three mammalian BN receptors, and GRPR (BB_2_ or BRS2; 384 amino acids) is the only one that is well characterized. GRPR is a glycosylated, 7-transmembrane, G-protein–coupled receptor that, upon binding with its ligands, gives rise to a complex cascade of intracellular reactions. In the physiological state, GRPR is expressed at low levels in non-neuroendocrine tissues of the breast and pancreas, and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (6). On the contrary, GRPR is overexpressed in various tumors, establishing itself as an optimal target for theranostics (7-10).

To date, a large number of BN derivatives have been synthesized based on either truncated BN(6-14) or BN(7-14) or full-length BN(1-14) (4, 10, 11). The truncated BN analogs are generally more stable in vivo, but the full-length analogs offer more flexible labeling sites through the amino acids 1 to 6. For most BN analogs, the amino acids on position 13 (Leu) and 14 (Met) have been replaced by unnatural amino acids, and Lys has been placed on position 3 for attachment of radiolabels. Spacers and chelators have also been widely used for conjugation purposes and for favorable kinetics.

In 2009, Fragogeorgi et al. reported two ^99m^Tc-labeled BN derivatives with different hydrophilicities and overall charges (12). One BN derivative, ^99m^Tc-N_3_S-BN(2-14), had a sequence of ^99m^Tc^(V)^O-Gly-Gly-Cys-bombesin(2-14). Another BN derivative, ^99m^Tc-BN-O or ^99m^Tc-N_3_S-X-BN(2-14), had the same sequence, but a basic amino acid spacer (X = Orn-Orn-Orn) was introduced. Both agents utilize the Gly-Gly-Cys as a tripeptide N_3_S-type chelator for radiolabeling, but ^99m^Tc-BN-O is more hydrophilic than ^99m^Tc-N_3_S-BN(2-14). Comparative studies have shown that hydrophilicity and charge strongly affect the binding properties and biodistribution patterns of the agents, and ^99m^Tc-BN-O is superior to ^99m^Tc-N_3_S-BN(2-14) for use in imaging tumors. To understand whether presence of a positively charged and highly polar spacer is critical for body clearance, the same group of investigators recently developed the agent ^99m^Tc-BN-A, which is a C-terminally amidated BN(2-14) analog with a positively charged, more polar natural spacer (Arg)_3_ than the spacer (Orn)_3_ (1). Liolios et al. investigated the in vitro and in vivo properties of ^99m^Tc-BN-A and compared to the properties of ^99m^Tc-BN-O (1). This chapter summarizes the comparative data obtained by Liolios et al. with ^99m^Tc-BN-A and ^99m^Tc-BN-O (1). The data obtained with ^99m^Tc-N_3_S-BN(2-14) and ^99m^Tc-BN-O by Fragogeorgi et al. can be reviewed in the chapter on ^99m^Tc-N_3_S-X-BN(2-14) (http://www.ncbi.nlm.nih.gov/books/NBK23708/) in MICAD.

### Related Resource Links:

- Protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) information for GRPR
- Structure information of BN and analogs in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=bombesin)
- GRPR-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=GRPR%20AND%20micad%5bbook%5d)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22459664)]

The BN peptides (Arg)_3_-bombesin(2-14) (BN-A) and (Orn)_3_-bombesin(2-14) (BN-O) were synthesized on a Rink-amide resin following the Fmoc strategy (1). The chemical purity for both BN-A and BN-O was >95%. Pure BN-A was obtained at a yield of ~39%, while introduction of the (Orn)_3_ spacer in BN-O led to a significant reduction in yield (~9%). The two peptides presented a retention time (Rt) difference of 1.8 min in reverse-phase high-performance liquid chromatography (RP-HPLC), with BN-O eluting earlier than BN-A. ^185/187^Re-A-BN and ^185/187^Re-O-BN were prepared by ligand exchange reactions for 2 h at 67°C, starting from the ^185/187^Re^(V)^O gluconate precursor. Radiolabeling with ^99m^Tc was performed by radioisotope exchange from the ^99m^Tc^(V)^O gluconate precursor for 30 min at 45°C . Sodium gluconate was used as an intermediate exchange ligand for ^99m^Tc, and stannous chloride was used as a reducing agent. The radiochemical yield of both ^99m^Tc-BN-A and ^99m^Tc-BN-O was >98%. The stability for the two agents was tested up to 6 h after labeling, and both remained >90% intact. The Rts of ^185/187^Re- and ^99m^Tc-complexes were similar in RP-HPLC, indicating that ^185/187^Re and ^99m^Tc form complexes of similar structure. The specific activity was not reported.

The metabolic stability of ^99m^Tc-BN-A and ^99m^Tc-BN-O was studied in mouse plasma for 5, 15, 30, and 60 min at 37°C (1). Both agents presented similar metabolic patterns. After 5 min of incubation, 42.48 ± 1.45% of the ^99m^Tc-BN-A and 44.28 ± 3.84% of the ^99m^Tc-BN-O remained intact. One major radioactive metabolite for both agents was observed with Rt close to that of the corresponding intact peptides. This major metabolite probably contained a great part of the parent peptide chain, including the ^99m^Tc-conjugated chelator group. After 1 h incubation, ~15% of the ^99m^Tc-BN-A and ~18% of the ^99m^Tc-BN-O remained intact.

The metabolic stability of ^99m^Tc-BN-A and ^99m^Tc-BN-O was also studied in human plasma for 1 h at 37°C (1). The metabolic patterns observed in human plasma were similar to the patterns observed in mouse plasma, but the peptide degradation in human plasma was much slower. At 1 h, 60.2 ± 1.2% of the ^99m^Tc-BN-A and 63.0 ± 1.0% of the ^99m^Tc-BN-O remained intact. A radioactive metabolite with Rt close to that of the intact peptide was also present for both agents, but in a smaller amount in comparison to the metabolite in mouse plasma. This metabolite was clearly visible in the mouse plasma after the first 5 min of incubation, but 4%–5% was visible after 1 h incubation in the human plasma.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22459664)]

The GRPR-binding capabilities (IC_50_ values) of BN-A, BN-O, and their ^185/187^Re complexes were evaluated in GRPR-positive PC-3 cells with a competitive cell-binding assay, using [^125^I-Tyr^4^]-BN as the GRPR-specific radioligand and [Tyr^4^]-BN as the control compound (1). Liolios et al. observed a typical sigmoid curve for displacement of [^125^I-Tyr^4^]-BN from PC-3 cells as a function of increasing concentration of all five different cold ligands under study (i.e., [Tyr^4^]-BN, BN-A, BN-O, ^185/187^Re-BN-A, and ^185/187^Re-BN-O) (1). All compounds showed an affinity similar to that of the control peptide [Tyr^4^]-BN (Table 1). Addition of the positively charged amino acid spacer and the Gly-Gly-Cys chelator group did not affect the binding affinity of the BN analogs. The differences for the receptor-binding affinity between BN-A and BN-O as well as between their ^185/187^Re complexes were not significant.

Table 1. The IC_50_ values of the tested BN analogs.

Compound | IC_50_ (nM) | Standard error | Statistics
BN-A | 0.50 | 0.09 | N
^185/187^Re-BN-A | 1.58 | 0.16 | Y
BN-O | 0.46 | 0.04 | N
^185/187^Re-BN-O | 0.77 | 0.07 | Y
[Tyr^4^]-BN | 0.45 | 0.04 | –

Y: statistical difference from [Tyr^4^]-BN; N: no difference from [Tyr^4^]-BN.

The uptake (internalization) and efflux (externalization), as a function of time of the ^99m^Tc-BN-A and ^99m^Tc-BN-O under study, were assessed with PC-3 cells in the presence (blocking experiments) or absence of the corresponding native BN peptides (1). The internalization rate of ^99m^Tc-BN-A increased rapidly until 120 min after initialization of incubation with PC-3 cells. Between 90 min and 120 min, ^99m^Tc-BN-A internalization reached a plateau and remained stable for >3 h of incubation. Nonspecific internalization in the presence of native BN was stable at <5% during the whole experiment. ^99m^Tc-BN-O reached its plateau after the first 60 min of incubation. The specific and nonspecific internalization levels were similar for both agents.

The externalization rate was studied when the agents reached the maximum levels of internalization (1). Measurements up to 90 min after incubation showed that ~68% of the ^99m^Tc-BN-A remained trapped in the cells, similar to measurements of the ^99m^Tc-BN-O, indicating similar rates of externalization for both peptides.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22459664)]

The biodistribution of ^99m^Tc-BN-A and ^99m^Tc-BN-O was comparatively studied in healthy female Swiss mice at 5, 15, 30, 60, 90, and 120 min, respectively, after injection of 2.775–4.625 MBq (0.075–0.125 mCi) of each agent via the tail vein (number of mice not reported) (1). Results were expressed as percentage of injected dose per organ (% ID/organ) or per gram tissue (% ID/g). Blood was assumed to be 7% of the total body weight for total blood radioactivity calculation. Receptor-blocking studies were carried out with co-administration of an excess amount (1 mg/ml) of the corresponding native BN peptides, and animals were euthanized at 30 min after co-injection.

Biodistribution studies showed that both agents cleared quickly from blood (1). ^99m^Tc-BN-A had a higher blood value than ^99m^Tc-BN-O (9.47 ± 1.12 versus 4.92 ± 0.65% ID/g) at 5 min after injection and exhibited a faster blood clearance thereafter, with lower blood concentrations than ^99m^Tc-BN-O. The kinetic patterns of ^99m^Tc-BN-A at 5 min after injection were similar in most organs, including heart, lungs, and liver, exhibiting higher values (% ID/g) than those of ^99m^Tc-BN-O and rapidly decreasing thereafter. The uptake values of ^99m^Tc-BN-A in lungs and liver were 8.91 ± 0.87% and 9.90 ± 1.31% ID/g at 5 min after injection, respectively, and <5% ID/g at 15 min in lungs and at 30 min in liver. ^99m^Tc-BN-O remained <5% ID/g in lungs and liver during the whole experiment. The predominant excretion route for both agents was via the kidneys. The urine radioactivity for ^99m^Tc-BN-A reached 63.34% ID/organ at 60 min after injection, while a similar value (63.15% ID/organ) was observed for ^99m^Tc-BN-O at 120 min after injection. The ^99m^Tc-BN-O urine value was 30.58% ID/organ at 60 min after injection. The high kidney retention for both agents was considered to be related to the increase in their overall charge due to the presence of positively charged amino acids in their spacer chains. In the GRPR-positive pancreas, ^99m^Tc-BN-A exhibited a high uptake, with an initial value of 14.07 ± 2.18% ID/g and values of >9.0% ID/g until 120 min after injection. Accumulation for both agents peaked at ~24.0% ID/g in the pancreas at 15 min after injection. The uptake values in muscle, spleen, and stomach were insignificant for both agents.

The biodistribution of ^99m^Tc-BN-A and ^99m^Tc-BN-O was also studied in SCID mice bearing PC-3 tumors (number of mice not reported) (1). ^99m^Tc-BN-A showed a high blood value at 15 min after injection (7.14 ± 1.4% ID/g), which rapidly decreased within 60 min (0.8 ± 0.16% ID/g). ^99m^Tc-BN-A rapidly accumulated in the GRPR-positive PC-3 tumors (6.94 ± 0.50% ID/g at 15 min after injection) and pancreas (~24% ID/g at 15–30 min after injection). Blocking studies, performed at 30 min after co-administration of excess native BN, decreased accumulation of ^99m^Tc-BN-A in the tumor and pancreas. The predominant excretion route of both ^99m^Tc-BN-A and ^99m^Tc-BN-O in the PC-3 tumor-bearing mice was also via the kidneys. For ^99m^Tc-BN-A, the tumor/blood ratio increased until 120 min after injection, when it reached its highest value (4.53). The tumor/muscle ratio, which was high already at 15 min after injection (4.74), reached its peak at 30 min (8.86), decreased at 60 min (5.60), and increased again at 120 min after injection (8.65). The tumor/intestine ratio presented its highest value at 15 min after injection (2.0) and then decreased gradually until 120 min after injection (1.25). The tumor/kidney and tumor/liver ratios presented similar and stable values, which were also decreased at 120 min after injection. ^99m^Tc-BN-O presented a tumor/blood ratio of 1.86 at 30 min after injection, which increased to 33.32 at 120 min after injection. The tumor/kidney ratio was higher for ^99m^Tc-BN-A at 60 min after injection and lower at 30 min and 120 min after injection (0.39, 0.27, and 0.28, respectively) than the respective ratios of ^99m^Tc-BN-O (0.28, 0.52, and 0.48 at the same time points). The tumor/muscle ratio was higher for ^99m^Tc-BN-A than for ^99m^Tc-BN-O until 30 min after injection (8.86 versus 6.38) and decreased to values lower than those of ^99m^Tc-BN-O thereafter. Tumor/liver ratios for ^99m^Tc-BN-A were lower at all time points than the ratios for ^99m^Tc-BN-O. Tumor/intestine ratios for ^99m^Tc-BN-A were marginally higher than those for ^99m^Tc-BN-O at 120 min after injection (1.25 versus 1.17), while for all other time points the ratios were lower.

Imaging studies were performed with γ-ray scintigraphy in PC-3 tumor-bearing mice at 120 min after injection of ~7.4 MBq (~0.2 mCi) ^99m^Tc-BN-A (number of mice not reported) (1). The PC-3 tumor was visible as early as 10 min with clear contrast from the adjacent background and remained observable up to 60 min after injection. High radioactivity was observed in the kidneys and urinary bladder. Imaging analysis data were in agreement with the results obtained from the biodistribution study in PC-3 tumor-bearing mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Liolios C.C., Fragogeorgi E.A., Zikos C., Loudos G., Xanthopoulos S., Bouziotis P., Paravatou-Petsotas M., Livaniou E., Varvarigou A.D., Sivolapenko G.B. (2012). Structural modifications of (9)(9)mTc-labeled bombesin-like peptides for optimizing pharmacokinetics in prostate tumor targeting. Int J Pharm.
2 Maina T., Nock B.A., Zhang H., Nikolopoulou A., Waser B., Reubi J.C., Maecke H.R. (2005). Species differences of bombesin analog interactions with GRP-R define the choice of animal models in the development of GRP-R-targeting drugs. J Nucl Med.
3 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
4 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
5 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
6 Weber H.C. (2009). Regulation and signaling of human bombesin receptors and their biological effects. Curr Opin Endocrinol Diabetes Obes.
7 Yang Y.S., Zhang X., Xiong Z., Chen X. (2006). Comparative in vitro and in vivo evaluation of two 64Cu-labeled bombesin analogs in a mouse model of human prostate adenocarcinoma. Nucl Med Biol.
8 Liu S., Edwards D.S., Barrett J.A. (1997). 99mTc labeling of highly potent small peptides. Bioconjug Chem.
9 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
10 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
11 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
12 Fragogeorgi E.A., Zikos C., Gourni E., Bouziotis P., Paravatou-Petsotas M., Loudos G., Mitsokapas N., Xanthopoulos S., Mavri-Vavayanni M., Livaniou E., Varvarigou A.D., Archimandritis S.C. (2009). Spacer site modifications for the improvement of the in vitro and in vivo binding properties of (99m)Tc-N(3)S-X-bombesin[2-14] derivatives. Bioconjug Chem.